# ^99m^Tc/^188^Re-Labeled dipicolylamine-alendronate

Chemical name: | ^99m^Tc/^188^Re-Labeled dipicolylamine-alendronate | [image]
Abbreviated name: | [^99m^Tc/^188^Re]DPA-alendronate | [image]
Synonym: | | [image]
Agent Category: | Compound | [image]
Target: | Hdroxyapatite for bone imaging Molecular target: Farnesyl disphosphate synthase (geranylgeranyl diphosphate synthase 1) | [image]
Target Category: | Enzyme | [image]
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging | [image]
Source of signal / contrast: | ^99m^Tc/^188^Re | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structure of [^99m^Tc]DPA-alendronate.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=dipycolylamine%20alendronate&cmd=DetailsSearch)]

Bisphosphonates (BPs) or nitrogen-containing bisphosphonates (NBP) are often used for the management of pain palliation and disorders related to skeletal tissue, including those arising from cancer metastases, because these compounds exhibit a very high affinity for hydroxyapatite (HA), a component of the bone matrix. These phosphonates tend to accumulate in osteoclasts at areas of increased bone metabolism by inhibiting the farnesyl diphosphate synthase, an important enzyme of the mevalonate pathway in the cell (1), as described by Drake et. al. (2). Several BPs and NBPs are available commercially for clinical use to treat different bone disorders, and there are ongoing clinical trials (http://clinicaltrials.gov/ct2/results?term=bisphosphonates) approved by the United States Food and Drug Administration to evaluate these compounds for the treatment of various bone ailments. In addition, BPs are often labeled with ^99m^Tc or ^186/188^Re and used for the imaging and treatment of bone metastases. However, these compounds have limitations primarily because they exist either as a mixture of anionic compounds with varying properties (e.g., ^99m^Tc-labeled methyl diphosphonate (MDP)) or are rapidly degraded (e.g., [^186/188^Re]MDP) under in vivo conditions, resulting in a reduced uptake at targeted bone areas and an increased accumulation in non-target soft tissue (3). The ^99m^Tc- or ^186/188^Re-labeled BPs were suggested to have these limitations because the compounds possess dual activities: one phosphonate group of the BP molecule acts as a radionuclide chelator, and the other phosphonate group binds to the target(s). Therefore, due to the close proximity of the two groups, one activity may be interfering with the other (3).

To circumvent problems associated with the radiolabeled BPs, investigators developed NBPs with two independent activities such that the nitrogen-containing part would only chelate the radiotracer and the BP part would target the bone (4, 5). These NBPs are produced by complex synthetic procedures, are usually obtained as enantomeric mixtures, and bind to plasma proteins (3). In an effort to produce a NBP that does not have these limitations, Torres Martin de Rosales et al. synthesized an easy-to-produce dipicolylamine-alendronate (DPA-alendronate), which has the radionuclide binding part separated from the BP by a spacer. After labeling the agent with ^99m^Tc ([^99m^Tc]DPA-alendronate), the investigators compared its biodistribution and use as an imaging agent against [^99m^Tc]MDP in normal Balb/c mice (3). In another study the investigators compared the ex vivo biodistribution and imaging characteristics of ^188^Re(CO)_3_-labeled DPA-alendronate ([^188^Re(CO)_3_]-alendronate) to those of clinically approved ^188^Re-hydroxyethylidene-1,1-diphosphonate ([^188^Re]-HEDP) (6).

### Other sources of information

Protein and mRNA sequence (http://www.ncbi.nlm.nih.gov/nuccore/NM_001037277.1) of human farnesyl diphosphate synthase

Gene information (http://www.ncbi.nlm.nih.gov/gene/2224) regarding human farnesyl diphosphate synthase (GeneID: 2224)

Farnesyl diphosphate synthase in Online Mendelian Inheritance in Man (OMIM) (http://www.ncbi.nlm.nih.gov/omim/134629)

Structure of farnesyl diphosphate synthase (http://www.ncbi.nlm.nih.gov/Structure/mmdb/mmdbsrv.cgi?uid=59201) complexed with a bisphosphonate

Farnesyl diphosphate synthase in Kyoto Encyclopedia of Genes and Genomes (KEGG) Pathways (http://www.genome.jp/dbget-bin/www_bget?pathway+hsa00900)

Related chapters (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=Farnesyl+diphosphate+synthase++AND+micad%5Bbook%5D&doptcmdl=TOCView&log%24=booksrch&bname=micad) in MICAD

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=dipicolylamine-alendronate%20synthesis&cmd=DetailsSearch)]

The synthesis, characterization, and ^99m^Tc labeling of DPA-alendronate has been described by Torres Martin de Rosales et al. (3). The labeled product had a radiochemical yield of >98% (as determined with reversed-phase high-performance liquid chromatography (HPLC)) and a specific activity of 22 MBq/μg (594 μCi/μg). The radiochemical purity of the labeled compound was not reported. The production, radiochemical purity, yield, and specific activity of [^99m^Tc]MDP used in the various studies was not reported (3).

The synthesis, purification and labeling of [^188^Re(CO)_3_]-alendronate has been described by de Rosales et. al. (6). The radiochemical yield and specific activity of the labeled compound were reported to be ≥ 95% and 18.8 GBq/mg (507.6 mCi/mg), respectively. [^188^Re]-HEDP was synthesized as described elsewhere (7). The radiochemical yield of this compound was >97%. The purity and specific activity of [^188^Re]-HEDP was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=dipicolylamine-alendronate%20in%20vitro%20studies&cmd=DetailsSearch)]

[^99m^Tc]DPA-alendronate was reported to be stable in human plasma for at least 18 h (as determined with size-exclusion HPLC) and showed little binding to the serum proteins (3). Compared with [^99m^Tc]DPA-alendronate, [^99m^Tc]MDP was mostly bound to serum proteins during an incubation for 18 h with human serum as determined with an alcohol precipitation method (3).

An in vitro assay was used to compare the affinity and selectivity of [^99m^Tc]DPA-alendronate and [^99m^Tc]MDP for various calcium salts in the presence or absence of a non-radioactive DPA-alendronate (3). [^99m^Tc]DPA-alendronate was shown to have a high affinity for HA with >80% binding compared to [^99m^Tc]MDP, which exhibited ~40% binding to HA and calcium oxalate (CO), respectively. Presence of excess non-radioactive DPA-alendronate was reported to completely inhibit the binding of [^99m^Tc]DPA-alendronate to HA and CO (3).

The in vitro stability of [^188^Re(CO)_3_]-alendronate and [^188^Re]-HEDP was studied in phosphate buffered saline in a CO_2_ atmosphere at 37^o^C for 48 h (6). Under these conditions at 48 h after the incubation the former compound was 100% intact while only <30% of the latter compound remained intact as determined by thin layer chromatography. Stability of the two radiolabeled compounds was also studied in human serum under the same conditions described above. At the end of the 48 h incubation only [^188^Re(CO)_3_]-alendronate was reported to remain unbound to serum proteins and unmodified (as determined by size exclusion high performance liquid chromatography), but most of [^188^Re]-HEDP bound to the serum proteins and by 48 h >70% radioactivity from this radiochemical was lost into the free solution (6).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=dipicolylamine-alendronate%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^99m^Tc]DPA-alendronate (n = 4 animals) and [^99m^Tc]MDP (n = 3 animals) was studied in normal mice by injecting the radiotracers through the tail vein (3). After euthanization, the major organs were retrieved and counted in a gamma counter for the comparison of accumulated radioactivity from the two radiochemicals. Data obtained from the study were presented as percent injected dose per gram tissue (% ID/g). A high uptake of both tracers was observed in the bones (femur, 27–30% ID/g), and <3% ID/g was observed in all the soft tissue organs (lungs, liver, kidney, etc.). However, a higher amount of radioactivity was observed to accumulate in the liver and the lower gastrointestinal tract (2.5% ID/g) with [^99m^Tc]DPA-alendronate than with [^99m^Tc]MDP (0.4% ID/g).

Imaging was performed with a combination of single-photon emission computed tomography (SPECT) and computed tomography on Balb/C mice (n = 3 animals per radiocompound) over a 6-h period after injection of either [^99m^Tc]DPA-alendronate or [^99m^Tc]MDP through the tail vein (3). Uptake of both radiotracers was observed primarily in the bone joints where the metabolic activity is very high.

The ex vivo biodistribution of [^188^Re(CO)_3_]-alendronate and [^188^Re]-HEDP was respectively studied in groups of mice (n = 3 animals/group) as described by de Rosales et. al. (6). Compared to the femur, accumulation of both the radiochemicals in other major organs of the animals was negligible (<1%ID/g). Approximately 20%ID/g of [^188^Re(CO)_3_]-alendronate was detected in one whole femur of a group of animals compared to approximately 15%ID/g of [^188^Re]-HEDP in the other group.

In vivo imaging with [^188^Re(CO)_3_]-alendronate and [^188^Re]-HEDP using SPECT was performed on Balb/c mice (n = 3 animals/radiochemical) at 1, 5, 24 and 48 h after an intravenous administration of the respective radiochemicals through the tail vein (6). From the images it was clear that [^188^Re(CO)_3_]-alendronate accumulated mainly in the metabolically active areas of the bone such as the joints and only low levels of radioactivity was detected in the soft tissues. Although the uptake of [^188^Re]-HEDP increased only during the initial 5 h the uptake of [^188^Re(CO)_3_]-alendronate was observed to increase up to 24 h after the intravenous injection.

On the basis of observations from the above studies, the investigators concluded that [^99m^Tc/^188^Re]DPA-alendronate was a good bone-targeting (imaging and therapy) agent, but further evaluation was necessary for its use in humans as a diagnostic or a therapeutic agent for bone metastasis (3, 6).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=dipicolylamine-alendronate%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=dipicolylamine-alendronate%20Human%20Studies&cmd=DetailsSearch)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Kimmel D.B. (2007). Mechanism of action, pharmacokinetic and pharmacodynamic profile, and clinical applications of nitrogen-containing bisphosphonates. J Dent Res.
2 Drake M.T., Clarke B.L., Khosla S. (2008). Bisphosphonates: mechanism of action and role in clinical practice. Mayo Clin Proc.
3 Torres Martin de Rosales R., Finucane C., Mather S.J., Blower P.J. (2009). Bifunctional bisphosphonate complexes for the diagnosis and therapy of bone metastases. Chem Commun (Camb).
4 Ogawa K., Mukai T., Arano Y., Otaka A., Ueda M., Uehara T., Magata Y., Hashimoto K., Saji H. (2006). Rhemium-186-monoaminemonoamidedithiol-conjugated bisphosphonate derivatives for bone pain palliation. Nucl Med Biol.
5 Ogawa K., Mukai T., Inoue Y., Ono M., Saji H. (2006). Development of a novel 99mTc-chelate-conjugated bisphosphonate with high affinity for bone as a bone scintigraphic agent. J Nucl Med.
6 Torres Martin de Rosales R., Finucane C., Foster J., Mather S.J., Blower P.J. 188Re(CO)3-dipicolylamine-alendronate: a new bisphosphonate conjugate for the radiotherapy of bone metastases. Bioconjug Chem.
7 Palmedo H., Guhlke S., Bender H., Sartor J., Schoeneich G., Risse J., Grunwald F., Knapp F.F., Biersack H.J. (2000). Dose escalation study with rhenium-188 hydroxyethylidene diphosphonate in prostate cancer patients with osseous metastases. Eur J Nucl Med.